# 3-N-[^11^C]Methylspiperone

Chemical name: | 3-N-[^11^C]Methylspiperone
Abbreviated name: | [^11^C]NMSP
Synonym:
Agent Category: | Compound
Target: | 5-HT_2A_ serotonin receptor, dopamine D_2/3_ receptors
Target Category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal / contrast: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents; - Non-primate non-rodent mammals; - Non-human primates; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20and%203-N-methylspiperone)]

Dopamine, a neurotransmitter, plays an important role in the mediation of movement, cognition, and emotion (1, 2). Dopamine shortage plays a role in various neuropsychiatric disorders, such as Parkinson’s disease (PD), schizophrenia, autism, attention deficit hyperactivity disorder, and drug abuse. Two subtypes of dopamine receptors, D_1_ and D_2/3_, were well characterized pharmacologically and biochemically (3). D_2/3_ dopamine receptors have been implicated in the pathophysiology of PD, Alzheimer's disease, Huntington’s disease (HD), and schizophrenia (4).

Serotonin (5-hydroxytryptamine, 5-HT) has diverse physiological roles as a neurotransmitter in the central nervous system (5). It also is a regulator of smooth muscle function and platelet aggregation. The brain cortical 5-HT system has been implicated in several neuropsychiatric disorders, including major depression, anxiety, obsessive-compulsive disorder, and schizophrenia (6, 7).

Spiperone and its analog, 3-N-methylspiperone (NMSP), are high-affinity D_2/3_ dopamine and 5-HT_2A_ serotonin receptor antagonists, showing a low affinity for α_1_-adrenergic receptors (8, 9). 3-N-[^11^C]Methylspiperone ([^11^C]NMSP) has been studied as a positron emission tomography (PET) tracer for imaging D_2/3_ and 5HT_2A_ receptor densities.

### Related Resource Links:

- Chapters in MICAD (5-HT_2A_ (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=5-HT2A+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad), Dopamine receptors (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=dopamine%20(receptors%20OR%20receptor)+%20AND+Table+AND+micad%5Bbook%5D))
- Gene information in NCBI (5-HT_2A_ (http://www.ncbi.nlm.nih.gov/gene/3356), D_2_ receptor, (http://www.ncbi.nlm.nih.gov/gene/1813) D_3_ receptor (http://www.ncbi.nlm.nih.gov/gene/1814))
- Articles in Online Mendelian Inheritance in Man (OMIM) (5-HT_2A_ (http://www.ncbi.nlm.nih.gov/omim/182135), D_2_ receptor (http://www.ncbi.nlm.nih.gov/omim/126450), D_3_ receptor (http://www.ncbi.nlm.nih.gov/omim/126451))
- Clinical trials (5-HT_2A_ (http://www.clinicaltrials.gov/ct2/results?term=5-HT2A), Dopamine receptors (http://www.clinicaltrials.gov/ct2/results?term=dopamine+receptor))
- Drug information in Food and Drug Administration (5-HT_2A_ (http://google2.fda.gov/search?q=5-HT2a&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=8&y=1), Dopamine receptors (http://google2.fda.gov/search?q=dopamine+receptor&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=6&y=12))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2811C%20and%203-N-methylspiperone%29%20and%20synthesis)]

A continuous flow procedure was used for the synthesis of [^11^C]methyl iodide from [^11^C]CO_2_. Alkylation of the amide nitrogen in spiperone in tetrabutylammonium hydroxide solution by [^11^C]methyl iodide provided [^11^C]NMSP in 20-40% radiochemical yield against [^11^C]CO_2_ in 40 min (10). [^11^C]NMSP was purified by high-performance liquid chromatography (HPLC). The specific activity was 10 GBq/μmol (270 mCi/μmol) at the end of synthesis (EOS). Omokawa et al. (11) and Dannals et al. (12) reported the time required for the synthesis and purification of [^11^C]NMSP from [^11^C] CO_2_ and spiperone to be 20-21 min with radiochemical yields of 21-35%. [^11^C]NMSP has been prepared automatically with a high specific activity (37 ± 18 GBq/μmol or 1 Ci/μmol at EOS) at 98.3 ± 1.0% radiochemical purity in 29 min of total synthesis time (13).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2811C%20and%203-N-methylspiperone%29%20and%20in%20vitro)]

NMSP was reported to have selective binding affinity to D_2_ (striatum) and 5-HT_2A_ (frontal cortex) receptor sites in homogenates of rat brain membranes (14). The K_d_ value of [^3^H]NMSP was 0.28 nM when the 5-HT_2A_ binding sites in the striatum were blocked by 40 nM ketanserin and 0.32 nM without blocking. The K_d_ value of [^3^H]raclopride was 2.08 nM. The D_2_ receptor binding density (B_max_) was almost identical for both radioligands (20 fmol/mg tissue). The B_max_ of [^3^H]NMSP for 5-HT_2A_ in the frontal cortex was 6.8 fmol/mg (35% of the total binding).

Using human putamen homogenates, the K_d_ values of [^3^H]NMSP and [^3^H]raclopride were 0.16 nM (0.22 nM in the presence of ketanserin) and 3.89 nM, respectively (14). The D_2_ receptor binding density (B_max_) was almost identical for both radioligands (10 fmol/mg tissue). The B_max_ of [^3^H]NMSP for 5-HT_2A_ was 3.3 fmol/mg tissue (30% of the total binding). The dissociation half-life values as measured by the addition of (+)-butaclamol were 14.8 and 1.19 min with [^3^H]NMSP and [^3^H]raclopride, respectively. NMSP was found to block the binding of [^3^H]raclopride competitively, whereas raclopride blocked the binding of [^3^H]NMSP both competitively and noncompetitively. Dopamine was found to be more potent in inhibiting [^3^H]raclopride than inhibiting [^3^H]NMSP binding to D_2_ receptors, partly because of the lower affinity of raclopride.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2811C%20and%203-N-methylspiperone%29%20and%20rodentia)]

Biodistribution studies in mice showed a high accumulation of radioactivity in the liver (9.98% injected dose (ID)/g) and kidneys (3.94% ID/g) at 30 min after injection of [^11^C]NMSP (15). The brain had a moderate uptake of 1.13% ID/g. The striatum had an uptake of 4.89% ID/g at 60 min with a striatum-to-cerebellum ratio of 20:1.

In the biodistribution studies in rats, there was a high accumulation of radioactivity in the liver, lung, and kidneys, whereas the brain radioactivity was not as high (16). The radioactivity in the striatum increased from 0.98% ID/g at 10 min to 1.9% at 60 min. On the other hand, the radioactivity in the cerebellum, which contains few or no D_2_ receptors, decreased from 0.29% at 10 min to 0.19% at 60 min. In the striatum, in vivo saturation and displacement studies estimated a B_max_ of 10-14 fmol/mg of tissue for [^11^C]NMSP and a K_d_ of 10-20 nmol/kg of body weight. Pretreatment of 5 mg/kg of spiperone 15 min before [^11^C]NMSP injection caused more inhibition than 15 min after [^11^C]NMSP injection. This indicated that [^11^C]NMSP bound tightly to its receptor sites in the striatum.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2811C%20and%203-N-methylspiperone%29%20and%20%28dog%20or%20pig%20or%20rabbit%20or%20sheep%29)]

Using PET, Rosa-Neto et al. (17) reported the binding potentials (PBs, ratios of B_max_ to K_d_) of [^11^C]raclopride and [^11^C]NMSP in brain of living pigs, first in a baseline condition and then at 45 and 165 min after intravenous infusion of methylenedioxymethamphetamine (MDMA, "Ecstasy") (1 mg/kg). Concomitant studies of cerebral blood flow did not reveal significant perfusion changes in the cerebellum reference region or in striatum. Relative to the baseline PB of [^11^C]raclopride for dopamine D_2_ receptors in striatum (PB = 1.5-2.2), MDMA treatment reduced PB by 35% in the first post-treatment scan and by 22% in the second post-treatment scan. However, the baseline PB of [^11^C]NMSP for dopamine D_2_ and 5-HT_2A_ receptors in striatum (PB = 4-5) was decreased by 30% in the first scan and by 50% in the second scan. Therefore, a simultaneous release of dopamine and serotonin induced by MDMA in brain may account for the progressive decline in the availability of [^11^C]NMSP binding sites in striatum.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2811C%20and%203-N-methylspiperone%29%20and%20%28primate%20not%20human%29)]

[^11^C]NMSP PET studies in non-human primates have provided useful assessments of the D_2_ and 5-HT_2A_ receptors in the brain [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2811C%20and%203-N-methylspiperone%29%20and%20%28primate%20not%20human%29)]. Eckernas et al. (18) showed a selective uptake in putamen (7.16% ID/cm^3^) over the frontal cortex (1.68% ID/cm^3^) and in the cerebellum (0.94% ID/cm^3^) in baboon brains at 60 min after injection. The striatum [^11^C]NMSP retention was blocked by pretreatment with excess unlabeled NMSP (0.075 mg/kg).

Clozapine, a neuroleptic drug in the treatment of schizophrenia by dopamine receptor blockade, blocked [^11^C]NMSP accumulation in the striatum of a monkey pretreated with 0.3 and 3 mg/kg of clozapine (19). D-Amphetamine is known to induce a marked release of dopamine to the synaptic cleft (20). D-Amphetamine administration to monkeys decreased [^11^C]raclopride binding by 31.2 ± 8.1% but only by 6.0 ± 17.5% in [^11^C]NMSP binding in the striatum (21). [^11^C]NMSP was not sensitive enough to detect the change in dopamine levels induced by D-amphetamine in this study.

Using a system to study conscious monkeys, a significant increase in accumulation of [^11^C]NMSP was observed in the striatum of monkeys administered with ketamine (5 mg/kg) compared with the level in the conscious state, whereas no significant change was observed in the frontal cortex and cerebellum (22). This dose of ketamine caused sedation accompanied by psychotic symptoms, such as nystagmus and stereotyped movements of extremities. Kinetic analysis revealed that the value of the association constant for [^11^C]NMSP binding in the striatum was increased to approximately 130% by ketamine compared with the control values. Furthermore, the release of dopamine from the striatum measured by microdialysis was not affected by ketamine anesthesia. It was concluded that ketamine facilitates striatal dopaminergic neurotransmission through increasing the binding activity of dopamine D_2_ receptors in the striatum, suggesting that these changes may be related to the psychotomimetic behavioral symptoms of this drug. In a later study in monkeys, it was found that [^11^C]NMSP binding was increased, whereas [^11^C]raclopride binding was decreased with ketamine (23).

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2811C%20and%203-N-methylspiperone%29%20and%20human)]

[^11^C]NMSP studies of D_2_ receptor distribution in human brain were reported, showing a localization of radioactivity in the striatum. Gjedde and Wong (24) reported on [^11^C]NMSP PET studies in 14 patients with schizophrenia, 5 patients with manic depression, and 15 normal subjects (3 old men and 12 young men). In the young normal volunteers, a B_max_ of 17 pmol/g tissue was estimated in the caudate, with a K_i_ of 3 nM for haloperidol. The B_max_ values for the older normal men, manic-depressive men, drug-naïve schizophrenic patients, and drug-treated schizophrenic patients were 6, 21, 39, and 41 pmol/g, respectively. Other [^11^C]NMSP PET studies also confirmed the age-related decrease of D_2_ receptor density in the caudate nucleus and putamen (25, 26) and the elevated level of striatal D_2_ receptor density in patients with chronic schizophrenia as compared with controls (27). However, Farde et al. (28) found that there was little difference in D_2_ receptor density in schizophrenic patients and normal subjects using [^11^C]raclopride, indicating that there may be some important differences in the binding properties and selectivity of the two tracers. In 21 patients with HD, there was a significant reduction in relative binding of [^11^C]NMSP to D_2_ receptor sites in the caudate nucleus and putamen of HD patients as compared with 8 normal subjects at risk for HD (29). There was a correlation of [^11^C]NMSP binding in the caudate with motor functions. The [^11^C]NMSP binding in the putamen correlated with the duration of the illness.

Effect of risperidone (a high-affinity 5-HT_2A_ and D_2_ antagonist) on 5-HT_2A_ receptor occupancy was studied in 3 normal healthy volunteers by [^11^C]NMSP PET (30). There was 60% 5-HT_2A_ receptor occupancy ([^11^C]NMSP) in the neocortical regions and 50% D_2_ receptor occupancy ([^11^C]raclopride) in the putamen after oral administration of 1 mg of risperidone. In a later study with 6 schizophrenic patients, D_2_ receptor occupancy was 82% and 5-HT_2A_ receptor occupancy was 95% at 6-mg/day doses for 4 weeks (31). All six patients had extrapyramidal side effects. Subsequently, when the dose was reduced to 3 mg/day for 2 weeks, D_2_ receptor occupancy was 72% and 5-HT_2A_ receptor occupancy was 83%. Three patients had extrapyramidal side effects.

[^11^C]NMSP PET is useful for objective monitoring of D_2_ and 5-HT_2A_ receptor occupancy and density in patients being treated with antipsychotic drugs. Internal dosimetry data for [^11^C]NMSP in humans are not available in the literature.

## References

1 Carbon M., Ghilardi M.F., Feigin A., Fukuda M., Silvestri G., Mentis M.J., Ghez C., Moeller J.R., Eidelberg D. (2003). Learning networks in health and Parkinson's disease: reproducibility and treatment effects. Hum Brain Mapp.
2 Chesselet M.F., Delfs J.M. (1996). Basal ganglia and movement disorders: an update. Trends Neurosci.
3 Stoof J.C., Kebabian J.W. (1984). Two dopamine receptors: biochemistry, physiology and pharmacology. Life Sci.
4 Seeman P., Bzowej N.H., Guan H.C., Bergeron C., Reynolds G.P., Bird E.D., Riederer P., Jellinger K., Tourtellotte W.W. (1987). Human brain D1 and D2 dopamine receptors in schizophrenia, Alzheimer's, Parkinson's, and Huntington's diseases. Neuropsychopharmacology.
5 Lucki I. (1998). The spectrum of behaviors influenced by serotonin. Biol Psychiatry.
6 Abi-Dargham A., Gandelman M.S., DeErausquin G.A., Zea-Ponce Y., Zoghbi S.S., Baldwin R.M., Laruelle M., Charney D.S., Hoffer P.B., Neumeyer J.L., Innis R.B. (1996). SPECT imaging of dopamine transporters in human brain with iodine-123-fluoroalkyl analogs of beta-CIT. J Nucl Med.
7 Charney D.S. (1998). Monoamine dysfunction and the pathophysiology and treatment of depression. J Clin Psychiatry.
8 Morgan D.G., Marcusson J.O., Finch C.E. (1984). Contamination of serotonin-2 binding sites by an alpha-1 adrenergic component in assays with (3H)spiperone. Life Sci.
9 Boy C., Klimke A., Holschbach M., Herzog H., Muhlensiepen H., Rota Kops E., Sonnenberg F., Gaebel W., Stocklin G., Markstein R., Muller-Gartner H.W. (1998). Imaging dopamine D4 receptors in the living primate brain: a positron emission tomography study using the novel D1/D4 antagonist [11C]SDZ GLC 756. Synapse.
10 Burns H.D., Dannals R.F., Langstrom B., Ravert H.T., Zemyan S.E., Duelfer T., Wong D.F., Frost J.J., Kuhar M.J., Wagner H.N. (1984). (3-N-[11C]methyl)spiperone, a ligand binding to dopamine receptors: radiochemical synthesis and biodistribution studies in mice. J Nucl Med.
11 Omokawa H., Tanaka A., Iio M., Nishihara Y., Inoue O., Yamazaki T. (1985). Synthesis of N-methyl and N-11C-methyl spiperone by phase transfer catalysis in anhydrous solvent. Radioisotopes.
12 Dannals R.F., Ravert H.T., Wilson A.A., Wagner H.N. (1986). An improved synthesis of (3-N-[11C]methyl)spiperone. Int J Rad Appl Instrum [A].
13 Suzuki K., Inoue O., Tamate K., Mikado F. (1990). Production of 3-N-[11C]methylspiperone with high specific activity and high radiochemical purity for PET studies: suppression of its radiolysis. Int J Rad Appl Instrum [A].
14 Hall H., Wedel I., Halldin C., Kopp J., Farde L. (1990). Comparison of the in vitro receptor binding properties of N-[3H]methylspiperone and [3H]raclopride to rat and human brain membranes. J Neurochem.
15 Barrio J.R., Satyamurthy N., Huang S.C., Keen R.E., Nissenson C.H., Hoffman J.M., Ackermann R.F., Bahn M.M., Mazziotta J.C., Phelps M.E. (1989). 3-(2'-[18F]fluoroethyl)spiperone: in vivo biochemical and kinetic characterization in rodents, nonhuman primates, and humans. J Cereb Blood Flow Metab.
16 Yanai K., Ido T., Ishiwata K., Hatazawa J., Watanuki S., Takahashi T., Ujiie A., Ito M., Matsuzawa T. (1986). Characteristics of specific in vivo labeling of neuroleptic binding sites with 3-N-[11C]methylspiperone. Eur J Nucl Med.
17 Rosa-Neto P., Gjedde A., Olsen A.K., Jensen S.B., Munk O.L., Watanabe H., Cumming P. (2004). MDMA-evoked changes in [11C]raclopride and [11C]NMSP binding in living pig brain. Synapse.
18 Eckernas S.A., Aquilonius S.M., Hartvig P., Hagglund J., Lundqvist H., Nagren K., Langstrom B. (1987). Positron emission tomography (PET) in the study of dopamine receptors in the primate brain: evaluation of a kinetic model using 11C-N-methyl-spiperone. Acta Neurol Scand.
19 Hartvig P., Eckernas S.A., Lindstrom L., Ekblom B., Bondesson U., Lundqvist H., Halldin C., Nagren K., Langstrom B. (1986). Receptor binding of N-(methyl-11C) clozapine in the brain of rhesus monkey studied by positron emission tomography (PET). Psychopharmacology (Berl).
20 Innis R.B., Malison R.T., al-Tikriti M., Hoffer P.B., Sybirska E.H., Seibyl J.P., Zoghbi S.S., Baldwin R.M., Laruelle M., Smith E.O., et al. (1992). Amphetamine-stimulated dopamine release competes in vivo for [123I]IBZM binding to the D2 receptor in nonhuman primates. Synapse.
21 Hartvig P., Torstenson R., Tedroff J., Watanabe Y., Fasth K.J., Bjurling P., Langstrom B. (1997). Amphetamine effects on dopamine release and synthesis rate studied in the Rhesus monkey brain by positron emission tomography. J Neural Transm.
22 Onoe H., Inoue O., Suzuki K., Tsukada H., Itoh T., Mataga N., Watanabe Y. (1994). Ketamine increases the striatal N-[11C]methylspiperone binding in vivo: positron emission tomography study using conscious rhesus monkey. Brain Res.
23 Kobayashi K., Inoue O., Watanabe Y., Onoe H., Langstrom B. (1995). Difference in response of D2 receptor binding between 11C-N-methylspiperone and 11C-raclopride against anesthetics in rhesus monkey brain. J Neural Transm Gen Sect.
24 Gjedde A., Wong D.F. (1987). Positron tomographic quantitation of neuroreceptors in human brain in vivo--with special reference to the D2 dopamine receptors in caudate nucleus. Neurosurg Rev.
25 Wagner H.N. (1985). Radiolabeled drugs as probes of central nervous system neurons. Clin Chem.
26 Wong D.F., Wagner H.N., Dannals R.F., Links J.M., Frost J.J., Ravert H.T., Wilson A.A., Rosenbaum A.E., Gjedde A., Douglass K.H., et al. (1984). Effects of age on dopamine and serotonin receptors measured by positron tomography in the living human brain. Science.
27 Tune L.E., Wong D.F., Pearlson G., Strauss M., Young T., Shaya E.K., Dannals R.F., Wilson A.A., Ravert H.T., Sapp J., et al. (1993). Dopamine D2 receptor density estimates in schizophrenia: a positron emission tomography study with 11C-N-methylspiperone. Psychiatry Res.
28 Farde L., Wiesel F.A., Hall H., Halldin C., Stone-Elander S., Sedvall G. (1987). No D2 receptor increase in PET study of schizophrenia. Arch Gen Psychiatry.
29 Brandt J., Folstein S.E., Wong D.F., Links J., Dannals R.F., McDonnell-Sill A., Starkstein S., Anders P., Strauss M.E., Tune L.E., et al. (1990). D2 receptors in Huntington's disease: positron emission tomography findings and clinical correlates. J Neuropsychiatry Clin Neurosci.
30 Nyberg S., Farde L., Eriksson L., Halldin C., Eriksson B. (1993). 5-HT2 and D2 dopamine receptor occupancy in the living human brain. A PET study with risperidone. Psychopharmacology (Berl).
31 Nyberg S., Eriksson B., Oxenstierna G., Halldin C., Farde L. (1999). Suggested minimal effective dose of risperidone based on PET-measured D2 and 5-HT2A receptor occupancy in schizophrenic patients. Am J Psychiatry.